# ^111^In-Diethylenetriaminepentaacetic acid-trastuzumab

Chemical name: | ^111^In-Diethylenetriaminepentaacetic acid-trastuzumab
Abbreviated name: | ^111^In-DTPA-humAb4D5-8
Synonym: | ^111^In-Herceptin^®^, ^111^In-anti-HER2 MAb, ^111^In-DTPA-trastuzumab.
Agent Category: | Antibody
Target: | Human epidermal growth factor receptor 2 (HER2)
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=119533), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=183984) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-trastuzumab%20OR%20111In-Herceptin%29)]

^111^In-Diethylenetriaminepentaacetic acid-trastuzumab (^111^In-DTPA-humAb4D5-8), which is formed by the conjugation of ^111^In with an intact recombinant humanized monoclonal antibody (MAb) against the antigen of human epidermal growth factor receptor 2 (HER2), has been developed for imaging of human breast cancer (1).

The epidermal growth factor receptors (HER/erbB) with tyrosine kinase activity are involved in transmission of signals controlling normal cell development, growth, differentiation, and survival (1-3). This cell-surface receptor family consists of four distinct members, the epidermal growth factor receptors HER1, HER2, HER3, and HER4. These receptors are found in various combinations in different tissues. There are nine ligands that bind directly to HER1, HER3, or HER4. HER2 can be activated as a result of ligand binding to other HER receptors. The ligandless HER2 receptor is encoded by the human gene HER2/c-erbB2 (HER2/neu). It has been found to be overexpressed in a wide variety of human cancers and in 20-30% of primary breast cancers (4). This overexpression is associated with aggressive tumor growth and metastatic activity. In breast cancer, HER2/neu gene amplification can result in 10- to 100-fold higher HER2 protein levels in tumor cells than that in normal breast epithelium. HER2 overexpression is considered a negative prognostic indicator for breast cancer.

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (5-7). Anti-HER2 MAbs have been generated for inhibiting the growth of tumor cells that possess activated HER2/neu receptors (8). Murine 4D5 MAb was raised against human breast and ovarian tumor cell lines overexpressing p185^HER2^. This MAb was found to recognize an extracellular epitope (amino acids 529 to 627) in the cysteine-rich II domain that resides very close to the transmembrane region (8). Murine 4D5 MAb was fully humanized by Carter et al. (9) to generate the humAb4D5-8 MAb in an effort to improve the safety and tolerance of the antibody for clinical applications. Trastuzumab is of the IgG_1_ kappa class and binds to the recombinant HER2 extracellular domain with an affinity constant (K_d_) of 0.1 nM. Cardiotoxicity is the most serious complication of using trastuzumab in humans (4, 10). One potential application of a radiolabeled anti-HER2 MAb is the pretreatment imaging of breast cancer patients to predict the cardiotoxicity and therapeutic efficacy of unlabeled trastuzumab.

Various anti-HER2 MAbs have been labeled with ^131^I, ^125^I, ^111^In, ^86^Y, ^90^Y, ^64^Cu, ^76^Br, or Gd for potential imaging and therapeutic applications (11-18). The labeling with radiometals is generally achieved by indirect labeling with use of a bifunctional chelating agent (19, 20). ^111^In, a photon emitter with a physical half-life (t_½_) of 2.8 days, is considered one of the radionuclides of choice for antibody imaging studies.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28111In%5BAll%20Fields%5D%20AND%20%28%22trastuzumab%22%5BSubstance%20Name%5D%20OR%20Trastuzumab%5BText%20Word%5D%29%29%20OR%20111In-Herceptin%5BAll%20Fields%5D%29%20AND)]

Trastuzumab was synthesized by humanization of murine 4D5 MAb (9). In this procedure, the complementarity-determining regions of the murine 4D5 MAb were transplanted into a human antibody model. A “gene conversion mutagenesis” strategy was used to simultaneously humanize the heavy- and light-chain region genes. A final “humanized” antibody, humAb4D5, containing only the antigen-binding loops from murine 4D5 MAb and human variable region framework residues plus IgG_1_ constant domains, was constructed. Of 8 humanized variants, humAb4D5-8 was found to bind its antigen 3-fold more tightly than the murine 4D5 MAb.

Lub-de Hooge et al. (1) described radiolabeling of the intact humAb4D5-8 MAb with ^111^In by conjugation using a modified cyclic diethylenetriamine pentaacetic acid (DTPA) anhydride method (1, 20). The initial DTPA conjugation was performed at a 1:1 molar ratio with 10 mg of humAb4D5-8 MAb in 1.4% sodium bicarbonate (pH 8, 200 µl) (1). Unbound DTPA was removed by ultrafiltration (twice for 30 min at 2,684g). The purified immunoconjugate, DTPA-humAb4D5-8 MAb, was either stored at −20 °C or used immediately for radiolabeling. Radiolabeled indium chloride (^111^InCl_3_; pH 1.5-1.9) solution was first buffered with an equal volume of 0.1 M sodium acetate to achieve a final pH of 5.5. The buffered ^111^InCl_3_ was then added to the DTPA-humAb4D5-8 MAb, and the reaction mixture was incubated at room temperature for 5 min. The labeling yield was 92.3 ± 2.3% (n = 4), and the radiochemical purity was 97.0 ± 1.5%. The specific activity of ^111^In-DTPA-trastuzumab was 18.5 MBq (0.5 mCi)/mg (2.8 GBq (0.075 Ci)/μmol based on a molecular weight of 150,000 for the intact MAb).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20in%20vitro)]

Lu-de Hooge et al. (1) determined the radioimmunoreactivity of ^111^In-DTPA-trastuzumab in cell-binding assays using HER2-overexpressing SK-OV-3 (human ovarian cancer) and SK-BR-3 (human breast cancer) cells. Both assays showed that the immunoreactive fraction was 0.87 ± 0.06 (n = 3). The nonspecific binding was less than 3%. An internalization assay with the SK-OV-3 cells showed that internalization was 25% after 1 h and 45% after 4 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20rodentia)]

Lu-de Hooge et al. (1) studied the biodistribution of ^111^In-DTPA-trastuzumab in mice bearing HER2-positive SK-OV-3 or HER2-negative GLC4 tumors. Each mouse with a 0.5-0.8 cm diameter s.c. tumor received an i.v. dose of 25 μg (0.2 ml) of MAb protein (450 ± 25 kBq (12.2 ± 0.68 μCi)). The tumor radioactivity uptakes (percentage injected dose (% ID)/g; n = 3-7) in mice with HER2-positive tumors were 9.77 ± 1.14, 13.71 ± 0.57, 16.30 ± 0.64, 15.29 ± 1.57, 8.31 ± 1.66, and 9.80 ± 3.22 at 5, 24, 48, 72, 96, and 168 h after injection, respectively. The tumor was best demonstrated in gamma imaging at 72 h after injection. The tumor radioactivity uptakes (% ID/g; n = 3-6) in the mice with HER2-negative tumors ranged from 3.17 ± 1.19 at 72 h to 5.70 ± 1.11 at 96 h. In the mice with HER2-positive tumors, the blood radioactivities (% ID/g) were 12.75 ± 1.50, 8.76 ± 0.46, 7.15 ± 0.69, 2.33 ± 0.46, 1.36 ± 0.51, and 1.63 ± 0.83 at 5, 24, 48, 72, 96, and 168 h after injection, respectively. At 5 h, the radioactivity uptakes (% ID/g) in well-perfused organs were 13.97 ± 2.52, 8.40 ± 1.67, 6.46 ± 0.47, 3.87 ± 1.00, and 3.83 ± 0.15 for the liver, spleen, kidney, lung, and heart, respectively. At 24 h, these values were 7.89 ± 1.80, 2.68 ± 0.48, 5.42 ± 0.58, 4.09 ± 0.69, and 1.90 ± 0.05% ID/g, respectively. No radioactivity was found in the brain, and the pancreas, stomach, bowel, bone, and skeletal muscle all demonstrated low uptake. A similar pattern of distribution was seen in mice bearing HER2-negative tumors. Metastases in the abdominal cavities of two mice with HER2-positive tumors also showed 15.4 and 11.2% ID/g at 24 and 96 h, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20human)]

Behr et al. (10) performed a preliminary single-photon emission computed tomography (SPECT) imaging study with ^111^In-DTPA-trastuzumab in 20 patients with metastatic breast cancer that expressed HER2. The radioactive tracer dose was coadministered with a loading dose of 4 mg of unlabeled trastuzumab. Subsequently, all patients were treated with unlabeled trastuzumab either as monotherapy (n = 4) or in combination with other chemotherapeutic agents. They reported that 7 of the 20 patients showed evidence of myocardial uptake. Six of these 7 patients reported cardiotoxicity after trastuzumab treatment, and the 7th patient suffered episodes of cardiac arrhythmia during trastuzumab administration. In contrast, the other 13 patients without myocardial uptake of ^111^In-DTPA-trastuzumab had reported no adverse cardiac effects. All 11 patients who showed intense tumor uptake of ^111^In-DTPA-trastuzumab had objective responses to trastuzumab therapy. The authors suggested that pretreatment imaging with ^111^In-DTPA-trastuzumab could predict the cardiotoxicity and therapeutic efficacy of unlabeled trastuzumab.

## References

1 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
2 Frankel C. Development and clinical overview of trastuzumab (herceptin) Semin Oncol Nurs 2000 16Suppl 14 13 7 11151453
3 Sliwkowski M.X. Lofgren J.A. Lewis G.D. Hotaling T.E. Fendly B.M. Fox J.A. Nonclinical studies addressing the mechanism of action of trastuzumab (Herceptin) Semin Oncol 1999 26Suppl 124 60 70 10482195
4 Slamon D.J., Leyland-Jones B., Shak S., Fuchs H., Paton V., Bajamonde A., Fleming T., Eiermann W., Wolter J., Pegram M., Baselga J., Norton L. (2001). Use of chemotherapy plus a monoclonal antibody against HER2 for metastatic breast cancer that overexpresses HER2. N Engl J Med.
5 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
6 Milenic D.E., Brechbiel M.W. (2004). Targeting of radio-isotopes for cancer therapy. Cancer Biol Ther.
7 Kowalsky R.J., Falen S.W. (2004). Radiopharmaceutcals in nuclear pharmacy and nuclear medicine. Second ed. , Washington, D.C.: APhA. 733-752.
8 Fendly B.M., Winget M., Hudziak R.M., Lipari M.T., Napier M.A., Ullrich A. (1990). Characterization of murine monoclonal antibodies reactive to either the human epidermal growth factor receptor or HER2/neu gene product. Cancer Res.
9 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
10 Behr T.M., Behe M., Wormann B. (2001). Trastuzumab and breast cancer. N Engl J Med.
11 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
12 Blend M.J., Stastny J.J., Swanson S.M., Brechbiel M.W. (2003). Labeling anti-HER2/neu monoclonal antibodies with 111In and 90Y using a bifunctional DTPA chelating agent. Cancer Biother Radiopharm.
13 Olafsen T., Kenanova V.E., Sundaresan G., Anderson A.L., Crow D., Yazaki P.J., Li L., Press M.F., Gambhir S.S., Williams L.E., Wong J.Y., Raubitschek A.A., Shively J.E., Wu A.M. (2005). Optimizing radiolabeled engineered anti-p185HER2 antibody fragments for in vivo imaging. Cancer Res.
14 Winberg K.J., Persson M., Malmstrom P.U., Sjoberg S., Tolmachev V. (2004). Radiobromination of anti-HER2/neu/ErbB-2 monoclonal antibody using the p-isothiocyanatobenzene derivative of the [76Br]undecahydro-bromo-7,8-dicarba-nido-undecaborate(1-) ion. Nucl Med Biol.
15 Xu F.J., Yu Y.H., Bae D.S., Zhao X.G., Slade S.K., Boyer C.M., Bast R.C., Zalutsky M.R. (1997). Radioiodinated antibody targeting of the HER-2/neu oncoprotein. Nucl Med Biol.
16 Palm S., Enmon R.M., Matei C., Kolbert K.S., Xu S., Zanzonico P.B., Finn R.L., Koutcher J.A., Larson S.M., Sgouros G. (2003). Pharmacokinetics and Biodistribution of (86)Y-Trastuzumab for (90)Y dosimetry in an ovarian carcinoma model: correlative MicroPET and MRI. J Nucl Med.
17 Tsai S.W., Sun Y., Williams L.E., Raubitschek A.A., Wu A.M., Shively J.E. (2000). Biodistribution and radioimmunotherapy of human breast cancer xenografts with radiometal-labeled DOTA conjugated anti-HER2/neu antibody 4D5. Bioconjug Chem.
18 Kobayashi H., Shirakawa K., Kawamoto S., Saga T., Sato N., Hiraga A., Watanabe I., Heike Y., Togashi K., Konishi J., Brechbiel M.W., Wakasugi H. (2002). Rapid accumulation and internalization of radiolabeled herceptin in an inflammatory breast cancer xenograft with vasculogenic mimicry predicted by the contrast-enhanced dynamic MRI with the macromolecular contrast agent G6-(1B4M-Gd)(256). Cancer Res.
19 Fritzberg A.R., Berninger R.W., Hadley S.W., Wester D.W. (1988). Approaches to radiolabeling of antibodies for diagnosis and therapy of cancer. Pharm Res.
20 Hnatowich D.J., Childs R.L., Lanteigne D., Najafi A. (1983). The preparation of DTPA-coupled antibodies radiolabeled with metallic radionuclides: an improved method. J Immunol Methods.